# [^111^In]-Labeled monovalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX

Chemical name: | [^111^In]-Labeled monovalent Fab fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX
Abbreviated name: | [^111^In]-DOTA-Fab-cG250
Synonym: | [^111^In]-DO3A-Fab-cG250; [^111^In]-Fab-cG250
Agent Category: | Antibody
Target: | Carbonic anhydrase IX
Target Category: | Enzyme
Method of detection: | Single-photon emission tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^111^In
Activation: | No
Studies: | - In vitro; - Rodents | Structure not available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[[underlined: PubMed]]

A common feature of most solid cancerous tumor types is the presence of hypoxic conditions (1) and the overexpression of carbonic anhydrase IX (CA IX), a transmembrane cell-surface enzyme that is known to regulate the pH and adhesion of tumor cells (2). Hypoxic tumors are often resistant to radio- and chemotherapy, have a high metastatic potential, and usually predict a poor outcome for the cancer patient (3). Although several methods (invasive and noninvasive) are available for the detection of hypoxia in tumors, including the use of radiolabeled small molecules, these methods are not completely reliable because they either yield variable diagnoses or have functional limitations due to incomplete penetration of tumors and fail to detect hypoxia in all tumor types (3, 4). Because CA IX is overexpressed in most solid tumors, it is considered to be a hypoxia biomarker, and targeting the CA IX for the detection of hypoxic tumors is of great interest to investigators (1, 3-5). A ^131^I-labeled murine monoclonal antibody (mAb) that targets the CA IX, designated G250, was developed and evaluated for the radiotherapy of metastatic renal cell carcinoma (RCC) patients, but no major responses were observed because the individuals developed immunity to the mAb (6). Subsequently, a ^131^I-labeled chimeric form of G250, [^131^I]-cG250, was developed and evaluated as an immunotherapeutic agent for the treatment of RCC (7). cG250 has been labeled with other nuclides (such as ^89^Zr, ^177^Lu, ^90^Y, etc.) and has been used in preclinical studies in rats (8) and for the treatment of RCC (7). However, only minor responses were observed in the clinical investigations, and dose escalation studies are ongoing (7).

Radiolabeled antibodies (Abs) have a limited ability to detect or treat cancer because these agents show only a peripheral penetration of solid tumors (due to a large size, ~150 kDa) and leave many neoplastic cells in the lesion untreated (9). In addition, Abs have prolonged blood circulation and present a high radiation dose risk to the bone marrow (10). In comparison, the smaller monovalent Fab (~50 kDa) and the divalent F(ab’)_2_ (~100 kDa) fragments derived from the parent Ab exhibit better tumor penetration and a shorter circulating half-life and are likely to yield better results if used to detect or treat solid malignant tumors (9). Between the two fragment types, the divalent F(ab’)_2_ fragments may be more useful for the detection or treatment of malignant tumors because they have a higher affinity for the antigen (11). With these observations in mind, a divalent F(ab’)_2_ fragment of cG250 was developed, labeled with ^131^I, and compared with the intact [^131^I]-cG250 Ab for its pharmacokinetic behavior and its ability to target tumors in mice and RCC patients (10). However, from this study the investigators concluded that the intact Ab was superior to the divalent fragment for targeting the RCC tumors. A clinical trial to investigate the safety of a ^124^I-labeled version of cG250 in patients with renal masses has been reported (12). In addition, cG250 is also under evaluation in several other clinical trials (http://clinicaltrials.gov/ct2/results?term=cG250). Recently, ^89^Zr-labeled F(ab’)_2_ fragments of cG250 were shown to be suitable for the visualization of hypoxic head and neck cancer xenograft tumors in mice (5).

Brouwers et al. compared the use of [^111^In]-isothiocynate-diethylenetriamine pentaacetic acid-cG250 and [^131^I]-cG250 for the detection of RCC metastases in five patients and concluded that the former tracer was superior to the latter for visualization of the tumors (13). In another study involving three patients, it was shown that neither ^131^I-labeled cG250 nor ^111^In-labeled cG250 were suitable for the radioimmunotherapy of biliary cancer (14). In a recent study using 1,4,7,10-tetraazacyclododecane-N,N’,N'',N’’’-tetraacetic acid (DOTA) as a nuclide conjugating agent, ^111^In-labeled cG250 Ab ([^111^In]-DOTA-cG250) and its Fab ([^111^In]-DOTA-Fab-cG250) and F(ab’)_2_ ([^111^In]-DOTA-F(ab’)_2_-cG250) fragments were generated and compared for their biodistribution and detection of hypoxic HT-29 cell (http://www.atcc.org/ATCCAdvancedCatalogSearch/ProductDetails/tabid/452/Default.aspx?ATCCNum=HTB-38&Template=cellBiology) (of human colorectal adenocarcinoma origin) xenograft tumors in mice (1).

This chapter details the studies performed with [^111^In]-DOTA-Fab-cG250. Studies performed with [^111^In]-DOTA-cG250 (15) and [^111^In]-DOTA-F(ab’)_2_-cG250 (16) are discussed in separate chapters of MICAD (www.micad.nih.gov).

### Other Sources of Information

Clinical trials (http://clinicaltrials.gov/ct2/results?term=Carbonic+anhydrase+IX+inhibitors) on carbonic anhydrase IX inhibitors

Human carbonic anhydrase IX in Entrez Gene (http://www.ncbi.nlm.nih.gov/gene/768) (Gene ID 768)

Protein and mRNA sequence (http://www.ncbi.nlm.nih.gov/nuccore/169636419) of human carbonic anhydrase IX

Crystal structure of the human carbonic anhydrase IX catalytic domain (http://www.ncbi.nlm.nih.gov/Structure/mmdb/mmdbsrv.cgi?uid=76607)

Human carbonic anhydrase IX in Online Mendelian Inheritance in Man (OMIM) (http://www.ncbi.nlm.nih.gov/nuccore?Db=omim&DbFrom=nuccore&Cmd=Link&LinkName=nuccore_omim&IdsFromResult=169636419) database

Hypoxia response in National Cancer Institute-Nature Pathways Interaction Database (http://pid.nci.nih.gov/search/pathway_landing.shtml?pathway_id=100145&pathway_name=hypoxia-inducible%20factor%20in%20the%20cardivascular%20system&source=BioCarta%20Imported&what=graphic&jpg=on&ppage=1)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20synthesis&cmd=DetailsSearch)]

The production and labeling of the cG250 Fab fragment with ^111^In was described in detail by Carlin et al. (1). On average, 1.9 ± 0.1 molecules of DOTA were reported to be conjugated to each molecule of Fab-cG250 (equal to 1.3% DOTA w/w). The ^111^In-labeling efficiency of the cG250 Fab fragment was >90% with a radiochemical purity of >99.9% and a specific activity of 370 MBq/mg (~1.5 Ci/mg).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20in%20vitro&cmd=DetailsSearch)]

Using SKRC-38 cells (of human RCC origin) under in vitro conditions, the immunoreactivity of [^111^In]-DOTA-Fab-cG250 was >90% with a B_max_ of 118,000 ± 21,000 binding sites/cell (1). Under the same experimental conditions, the B_max_ values for the cG250 and its F(ab’)_2_ fragment were 120,000 ± 22,000 and 114,000 ± 19,000 binding sites/cell, respectively (1). [^111^In]-DOTA-Fab-cG250 was reported to have a K_d_ of 14.05 ± 0.47 nM for the CA IX on the SKRC-38 cells. In comparison, the K_d_ values for the ^111^In-labeled cG250 and the F(ab’)_2_ fragment were 2.48 ± 0.04 and 1.76 ± 0.08 nM, respectively.

The tumor uptake of radioactivity from the labeled Fab, cG250, and the F(ab’)_2_ fragment was confirmed with ex vivo autoradiography of the tumor sections (1). In addition, the expression of CA IX and the occurrence of hypoxic conditions in the tumor sections were confirmed with immunohistochemical and pimonidazole staining procedures, respectively.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-cG250%20rodentia&cmd=DetailsSearch)]

The biodistribution of [^111^In]-DOTA-Fab-cG250 was studied in nu/nu nude mice (n = 4–5 animals/group per time point) bearing hypoxic HT-29 colorectal tumor xenografts as described by Carlin et al. (1). The animals were injected with the ^111^In-labeled Fab fragment through the tail vein and euthanized at preselected time points (ranging from 6 h to 7 days post-injection (p.i.)) to determine the amount of radioactivity accumulated in the tumors and the major organs. Data generated from the study were presented as percent injected dose per gram tissue (% ID/g).

The tumor uptake of radioactivity from the labeled Fab fragment was 3.6 ± 1.3% ID/g and 3.5 ± 1.7% ID/g at 6 h and 24 h p.i., respectively. The tumor/muscle (TM) and tumor/blood (TB) ratios with the labeled monovalent fragment were 4.8 and 2.8, respectively, at 6 h p.i., and these ratios increased to 6.7 and 16.6, respectively at 24 h p.i., which were lower than the ratios observed with [^111^In]-DOTA-cG250 at 7 days p.i. (see below). Compared with the labeled Fab fragment, the accumulation of radioactivity in the tumors with the ^111^In-labeled F(ab’)_2_ fragment was higher at the two time points, with 7.6 ± 1.4% ID/g and 9.3 ± 2.1% ID/g at 6 h and 24 h p.i., respectively. The TM and TB ratios with the divalent tracer were 8.9 and 4.6, respectively at 24 h p.i. The tumor uptake of ^111^In-labeled cG250 was 20.1 ± 4.8% ID/g at 2 days p.i. and increased to 26.4 ± 5.7% ID/g at day 7. In general, the tumor/non-tumor (TNT) ratios with [^111^In]-DOTA-cG250 increased for all tissues up to 7 days p.i., except for the liver and spleen, and little change in the TNT ratio for these organs was apparent during this period. At 7 days p.i., the TM and TB ratios with the labeled cG250 were 69 and 6.6, respectively, indicating a slow washout of radioactivity from these organs. The two Ab fragments showed ~10-fold lower tumor uptake and a similar increase in kidney accumulation of radioactivity compared with [^111^In]-DOTA-cG250. A high accumulation of radioactivity in the kidney was expected because the Fab and F(ab’)_2_ fragments (or their breakdown products) are known to be excreted through the urinary route and these organs are known to have a high expression of CA IX. These observations suggested that clearance of the [^111^In]-DOTA-Fab-cG250 and the [^111^In]-DOTA-F(ab’)_2_-cG250 fragments from blood was faster than that of the intact [^111^In]-DOTA-cG250 Ab. These results indicated that cG250 had a long circulation time compared with the Fab and F(ab’)_2_ fragments and that the tumor had a superior retention of the labeled Ab compared to either of its fragments. No blocking studies were reported.

From these studies, the investigators concluded that imaging with [^111^In]-DOTA-cG250 at 7 days p.i. was a better and more sensitive method for the detection of CA IX in hypoxic tumors in a murine model compared with its ^111^In-labeled Fab or F(ab’)_2_ fragments (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20non-primate%20mammals&cmd=DetailsSearch)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Non-Human%20Primates&cmd=DetailsSearch)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed?term=111In-DOTA-cG250%20Human%20Studies&cmd=DetailsSearch)]

No references are currently available.

## Supplemental Information

[Disclaimers]

No information is currently available.

## NIH Support

National Institutes of Health grants P01 CA115675, P01 CA033049, and P50 CA086438

## References

1 Carlin S., Khan N., Ku T., Longo V.A., Larson S.M., Smith-Jones P.M. (2010). Molecular targeting of carbonic anhydrase IX in mice with hypoxic HT29 colorectal tumor xenografts. PLoS One.
2 De Simone G., Supuran C.T. (2010). Carbonic anhydrase IX: Biochemical and crystallographic characterization of a novel antitumor target. Biochim Biophys Acta.
3 Michalski, M.H. and X. Chen, Molecular imaging in cancer treatment. Eur J Nucl Med Mol Imaging. 2010
4 Mees G., Dierckx R., Vangestel C., Van de Wiele C. (2009). Molecular imaging of hypoxia with radiolabelled agents. Eur J Nucl Med Mol Imaging.
5 Hoeben B.A., Kaanders J.H., Franssen G.M., Troost E.G., Rijken P.F., Oosterwijk E., van Dongen G.A., Oyen W.J., Boerman O.C., Bussink J. (2010). PET of hypoxia with 89Zr-labeled cG250-F(ab')2 in head and neck tumors. J Nucl Med.
6 Divgi C.R., Bander N.H., Scott A.M., O'Donoghue J.A., Sgouros G., Welt S., Finn R.D., Morrissey F., Capitelli P., Williams J.M., Deland D., Nakhre A., Oosterwijk E., Gulec S., Graham M.C., Larson S.M., Old L.J. (1998). Phase I/II radioimmunotherapy trial with iodine-131-labeled monoclonal antibody G250 in metastatic renal cell carcinoma. Clin Cancer Res.
7 Stillebroer A.B., Oosterwijk E., Oyen W.J., Mulders P.F., Boerman O.C. (2007). Radiolabeled antibodies in renal cell carcinoma. Cancer Imaging.
8 Brouwers A., Verel I., Van Eerd J., Visser G., Steffens M., Oosterwijk E., Corstens F., Oyen W., Van Dongen G., Boerman O. (2004). PET radioimmunoscintigraphy of renal cell cancer using 89Zr-labeled cG250 monoclonal antibody in nude rats. Cancer Biother Radiopharm.
9 Schmidt M.M., Wittrup K.D. (2009). A modeling analysis of the effects of molecular size and binding affinity on tumor targeting. Mol Cancer Ther.
10 Brouwers A., Mulders P., Oosterwijk E., Buijs W., Corstens F., Boerman O., Oyen W. (2004). Pharmacokinetics and tumor targeting of 131I-labeled F(ab')2 fragments of the chimeric monoclonal antibody G250: preclinical and clinical pilot studies. Cancer Biother Radiopharm.
11 Rudnick S.I., Adams G.P. (2009). Affinity and avidity in antibody-based tumor targeting. Cancer Biother Radiopharm.
12 Divgi C.R., Pandit-Taskar N., Jungbluth A.A., Reuter V.E., Gonen M., Ruan S., Pierre C., Nagel A., Pryma D.A., Humm J., Larson S.M., Old L.J., Russo P. (2007). Preoperative characterisation of clear-cell renal carcinoma using iodine-124-labelled antibody chimeric G250 (124I-cG250) and PET in patients with renal masses: a phase I trial. Lancet Oncol.
13 Brouwers A.H., Buijs W.C., Oosterwijk E., Boerman O.C., Mala C., De Mulder P.H., Corstens F.H., Mulders P.F., Oyen W.J. (2003). Targeting of metastatic renal cell carcinoma with the chimeric monoclonal antibody G250 labeled with (131)I or (111)In: an intrapatient comparison. Clin Cancer Res.
14 Hendrickx B.W., Punt C.J., Boerman O.C., Postema E.J., Oosterwijk E., Mavridu A., Corstens F.H., Oyen W.J. (2006). Targeting of biliary cancer with radiolabeled chimeric monoclonal antibody CG250. Cancer Biother Radiopharm.
15 Chopra, A., [111In]-Labeled chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.
16 Chopra, A., [111In]-Labeled divalent F(ab')2 fragment of chimeric monoclonal antibody cG250 directed against carbonic anhydrase IX. Molecular Imaging and Contrast agent Database (MICAD) [database online]. National Library of Medicine, NCBI, Bethesda, MD, USA. Available from www.micad.nih.gov, 2004 -to current.